# Gadolinium diethylenetriamine pentaacetic acid-Arg-Gly-Asp peptidomimetic

Chemical name: | Gadolinium diethylenetriamine pentaacetic acid-Arg-Gly-Asp peptidomimetic
Abbreviated name: | Gd-DTPA-g-mimRGD
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=mimRGD)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (2). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (3-8). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (7, 9, 10). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (11).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (12, 13). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (14-16); however, these Gd complexes did not proceed into further clinical development because of high tissue accumulation and slow excretion of toxic Gd ions. Furthermore, they are largely nonspecific. A low molecular weight, non-peptide, RGD mimetic (g-mimRGD, 5-{N'-[5-(4-Methylpyridin-2-ylamino)pentanoyl]hydrazino}-3-(4-biphenyl)-5-oxopentanoic acid trifluoroacetate) was identified to have good affinity and selectivity for the α_v_β_3_ integrin (50% inhibition concentration, 3 nM) (17). Burtea et al. (18) conjugated mimRGD to Gd-DTPA to form Gd-DTPA-g-minRGD for non-invasive in vivo MRI of α_v_β_3_ integrin expression in transgenic apolipoprotein E–deficient (ApoE^-/-^) mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd+mimRGD+synthesis)]

Solid-phase synthesis was used to prepare g-mimRGD, which was coupled to DTPA with the use of 2-(4-isothiocyanatobenzyl)-DTPA (p-SCN-Bn-DTPA) in aqueous solution (pH 10) (18). DTPA-g-mimRGD was isolated with column chromatography and complexed with GdCl_3_.6H_2_O. The mass of Gd-DTPA-g-mimRGD was confirmed with mass spectroscopy with one DTPA per g-mimRGD. The Gd complex exhibited proton longitudinal (r_1_) relaxivity values of 4.75 mM^-1^ s^-1^ at 0.47 T and 4.33 mM^-1^ s^-1^ at 1.5 T at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd+mimRGD+in+vitro)]

Burtea et al. (18) performed in vitro binding studies of Gd-DTPA-g-mimRGD in cultured human Jurkat T cells with R_1_ (longitudinal relaxation rate) MRI. Signal intensity was significantly higher (P < 0.01) with 0.4 mM Gd-DTPA-g-mimRGD than with 0.4 mM Gd-DTPA in Jurkat T cells with or without phorbol myristate acetate (PMA) stimulation. Co-incubation with 1.55 mM g-mimRGD inhibited the signal intensity by 36%. The R_1_ measured at 1.5 T exhibited superior binding levels (P < 0.05) of Gd-DTPA-g-mimRGD to PMA-stimulated cells (0.065 s^–1^) as compared with various controls, such as non-stimulated cells (0.023 s^–1^), Gd-DTPA (0.012 s^–1^ for PMA samples and 0.0075 s^–1^ for non-stimulated cells), or cells submitted to g-mimRGD competition (0.038 s^–1^). Gd-DTPA-g-mimRGD was found to be stable in blood plasma for up to 72 h of r_1_ measurements, and it did not interact with human serum albumin. Gd-DTPA-g-mimRGD exhibited a higher stability against transmetallation with Zn^2+^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd+mimRGD+rodentia)]

Burtea et al. (18) used a 4.7-T MRI scanner to perform in vivo MRI in ApoE^-/-^ mice (n = 10). Injection of Gd-DTPA-g-mimRGD (0.1 mmol/kg) provided strong enhancement in MRI contrast in the external structures of the aortic wall (tunica media and adventitia) within 10 min of injection; this enhancement was still visualized up to 90 min. On the other hand, Gd-DTPA provided only a diffuse contrast, and the aortic wall was not clearly outlined. Pretreatment with 0.1 mmol/kg Eu-DTPA-g-mimRGD inhibited the enhancement by 40% to 90% during the 90 min of scanning to nearly the same levels of contrast as control Gd-DTPA. Gd-DTPA-g-mimRGD exhibited a delayed clearance at 30 min and 60 min compared with Gd-DTPA. Immunohistochemical measurements of the excised aortas revealed the presence of various adhesion molecules in the aortas from the ApoE^-/-^ mice but not in the aortas from wild-type control mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd+mimRGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd+mimRGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd+mimRGD+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
5 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
6 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
7 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
8 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
9 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
10 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
11 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
12 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
13 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
14 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
15 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
16 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
17 Sulyok G.A., Gibson C., Goodman S.L., Holzemann G., Wiesner M., Kessler H. (2001). Solid-phase synthesis of a nonpeptide RGD mimetic library: new selective alphavbeta3 integrin antagonists. J Med Chem.
18 Burtea C., Laurent S., Murariu O., Rattat D., Toubeau G., Verbruggen A., Vansthertem D., Vander Elst L., Muller R.N. (2008). Molecular imaging of alpha v beta3 integrin expression in atherosclerotic plaques with a mimetic of RGD peptide grafted to Gd-DTPA. Cardiovasc Res.